# 4-[^18^F]Fluorobenzoyl-annexin V

Chemical name: | 4-[^18^F]Fluorobenzoyl-annexin V
Abbreviated name: | 4-[^18^F]FBA
Synonym: | [^18^F]Annexin V
Agent Category: | Protein
Target: | Phosphatidylserine, apoptosis and necrosis
Target Category: | Binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=468888), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4809273) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=308) for more information about annexin V.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20annexin%20V)]

Apoptosis (programmed cell death) plays an important role in the pathophysiology of many diseases, such as cancer, neurodegenerative disorders, vascular disorders, and chronic hepatitis, as well as in the biology of normal cells, such as epithelial cells and immune cells (1). Apoptosis is gene regulated (2) and is the result of proteolysis of intracellular components by activation of a series of proteolytic enzymes, called caspases, and changes of plasma membrane structure by translocase, floppase, and scramblase (3-5). As a result, there is rapid redistribution of phosphatidylserine (PS) from the inner membrane leaflet to the outer membrane leaflet, exposing the anionic head group of PS. On the other hand, PS is also accessible for annexin V binding in necrosis because of disruption of the plasma membrane.

Annexin V is a 36-kDa endogenous human protein produced, in particular, by epithelial cells from many tissues, such as the placenta, umbilical vessels, liver, spleen, kidney, heart, uterus, and skeletal muscle, as well as by erythrocytes, leukocytes, endothelial cells, and platelets (6). Annexin V binds to PS with high affinity (K_d_ = 7 nM) with 8 annexin V molecules per PS (3, 7, 8). Apoptosis can be induced by chemicals, radiation, cytokines, hormones, and various pathologic conditions (5); therefore, the ability to monitor apoptosis in association with disease progression or regression should provide important information for clinical applications. Annexin V has been radiolabeled with ^123^I, ^125^I, and ^99m^Tc for single photon imaging (9, 10). Recently, annexin V was successfully labeled with ^18^F (11, 12). ^18^F-labeled annexin V is being developed as a positron emission tomography (PET) agent for imaging apoptosis as well as necrosis. PET has a spatial resolution of 5-6 mm, which will permit better quantitation of small areas of apoptosis than can be achieved by single photon imaging (6-12 mm spatial resolution).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20annexin%20V%20and%20synthesis)]

4-[^18^F]Fluorobenzoyl-annexin V (4-[^18^F]FBA) was remotely synthesized via a computer-controlled, automated module within 90 min in a four-step procedure (12). Ethyl-4-[^18^F]fluorobenzoate was synthesized by nucleophilic fluorination of ethyl-4-(trimethylammonium)benzoate trifluoromethane-sulfonate, using the standard [^18^F]KF Kryptofix complex. Hydrolysis of ethyl-4-[^18^F]fluorobenzoate yielded 4-[^18^F]fluorobenzoic acid, which was then reacted with O-[N-succinimidyl]-N,N,N,N-tetramethyluronium tetrafluoroborate to form N-succinimidyl-4-[^18^F]fluorobenzoate. A free primary amino group of the annexin V molecule was coupled with N-succinimidyl-4-[^18^F]fluorobenzoate by a benzamido bond. The final product, 4-[^18^F]FBA, was eluted from a PD-10 cartridge with water. The overall radiochemical yield was in the range of 15-20% (corrected for decay) with a specific activity >35 GBq/μmol (0.95 Ci/μmol) and a radiochemical purity of 95%.

A manual four-step procedure was also used to synthesize 4-[^18^F]FBA via combination of 4-(dimethylamino)pyridine and N,N´-disuccinimidyl carbonate in the N-succinimidyl-4-[^18^F]fluorobenzoate formation step. The overall radiochemical yield was 17.6 ± 5.6% (corrected for decay), with a total synthesis time of 180 min, and the specific activity was 1.3-1.8 TBq/mmol (35-49 Ci/mmol) (11). The radiochemical purity was >95%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20annexin%20V%20and%20in%20vitro)]

In vitro binding studies of 4-[^18^F]FBA to PS liposomes showed that >96% of the radioactivity was found in the liposome after 10 min of incubation and 60 min of centrifugation (12). More than 98% of the bound radioactivity in the liposome was released into the medium by ethylenediaminetetraacetic acid, confirming that the binding of annexin V to PS is calcium dependent. 4-[^18^F]FBA was shown to selectively bind to apoptotic Jurkat T cells (induced by ultraviolet radiation) (12) and Ewing’s sarcoma TC32 cells (induced by etoposide) (11).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20annexin%20V%20and%20rodentia)]

Murakami et al. (13) performed biodistribution studies in normal rats and found high accumulation of radioactivity in the kidney (tissue/blood ratio of 15.8), followed by the spleen (3.0), liver (2.1), and heart (0.7) at 60 min after injection of 15 MBq (0.41 mCi, 10 μg) of 4-[^18^F]FBA. After injection of 15 MBq (0.41 mCi, 3 μg) of ^99m^Tc-annexin V into normal rats, the heart/blood ratio (0.9) was not significantly different from that for 4-[^18^F]FBA (0.7). However, the accumulation of ^99m^Tc-annexin V was significantly higher in the kidney (135.3), spleen (21.6), and liver (8.3). Therefore, the low accumulation of 4-[^18^F]FBA in these organs might be an advantage over ^99m^Tc-annexin V. In an ex vivo imaging experiment, 4-[^18^F]FBA was injected into rats 24 h after induction of myocardial ischemia. 4-[^18^F]FBA accumulated in the infarct area of the left ventricle, where apoptotic cells were observed. In separate experiments, 4-[^18^F]FBA or ^99m^Tc-annexin V was injected into ischemic or normal animals, and accumulation of 4-[^18^F]FBA and ^99m^Tc-annexin V in the infarct area was about 3-fold higher than in the non-infarct area.

Yagle et al. (14) performed more extensive biodistribution studies in normal rats and found high accumulation of radioactivity in the kidney (1.75% of injected dose (ID)/g), followed by the spleen (0.22% ID/g), lung (0.19% ID/g), bone (0.17% ID/g), liver (0.15% ID/g), and heart (0.057% ID/g) at 120 min after injection of 15-52 MBq (0.4-1.4 mCi) of 4-[^18^F]FBA. Nearly 70% of injected radioactivity was found in the urine. Pretreatment of rats with cycloheximide (5 mg/kg) to induce apoptosis in the liver significantly increased the accumulation of 4-[^18^F]FBA in the organ compared with untreated rats as measured by PET. Histologic staining of apoptotic cells showed increased apoptotic cells in the livers of rats that were treated with cycloheximide. The 3- to 9-fold increase in accumulation of 4-[^18^F]FBA was similar to terminal deoxynucleotide end-labeling (TUNEL) apoptotic cell assays (5- to 8-fold increase) performed with liver slices from rats treated with cycloheximide.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20annexin%20V%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20annexin%20V%20and%20%28primate%20not%20human%29)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20annexin%20V%20and%20human)]

No publications are currently available.

## NIH Support

CA42045, S10 RR17229

## References

1 Thompson C.B. (1995). Apoptosis in the pathogenesis and treatment of disease. Science.
2 Steller H. (1995). Mechanisms and genes of cellular suicide. Science.
3 Thiagarajan P., Tait J.F. (1990). Binding of annexin V/placental anticoagulant protein I to platelets. Evidence for phosphatidylserine exposure in the procoagulant response of activated platelets. J Biol Chem.
4 Song Z., Steller H. (1999). Death by design: mechanism and control of apoptosis. Trends Cell Biol.
5 Blankenberg F.G., Tait J., Ohtsuki K., Strauss H.W. (2000). Apoptosis: the importance of nuclear medicine. Nucl Med Commun.
6 Blankenberg F.G., Strauss H.W. (2001). Will imaging of apoptosis play a role in clinical care? A tale of mice and men. Apoptosis.
7 van Heerde W.L., de Groot P.G., Reutelingsperger C.P. (1995). The complexity of the phospholipid binding protein Annexin V. Thromb Haemost.
8 Tait J.F., Cerqueira M.D., Dewhurst T.A., Fujikawa K., Ritchie J.L., Stratton J.R. (1994). Evaluation of annexin V as a platelet-directed thrombus targeting agent. Thromb Res.
9 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
10 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
11 Toretsky J., Levenson A., Weinberg I.N., Tait J.F., Uren A., Mease R.C. (2004). Preparation of F-18 labeled annexin V: a potential PET radiopharmaceutical for imaging cell death. Nucl Med Biol.
12 Zijlstra S., Gunawan J., Burchert W. (2003). Synthesis and evaluation of a 18F-labelled recombinant annexin-V derivative, for identification and quantification of apoptotic cells with PET. Appl Radiat Isot.
13 Murakami Y., Takamatsu H., Taki J., Tatsumi M., Noda A., Ichise R., Tait J.F., Nishimura S. (2004). 18F-labelled annexin V: a PET tracer for apoptosis imaging. Eur J Nucl Med Mol Imaging.
14 Yagle K.J., Eary J.F., Tait J.F., Grierson J.R., Link J.M., Lewellen B., Gibson D.F., Krohn K.A. (2005). Evaluation of 18F-annexin V as a PET imaging agent in an animal model of apoptosis. J Nucl Med.